# ^123^I-Interleukin-2

Chemical name: | ^123^I-Interleukin-2
Abbreviated name: | ^123^I-IL-2
Synonym: | T cell growth factor
Agent Category: | Polypeptide
Target: | IL-2 receptors
Target Category: | Receptor binding
Method of detection: | SPECT, planar
Source of signal: | ^123^I
Activation: | No
Studies: | - In vitro; - Rodents; - Humans | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=28178861), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?val=NM_000586.2) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=Graphics&list_uids=3558) for more information about IL-2.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=123I%20and%20Interleukin-2)]

Interleukin-2 (IL-2) is a T-cell growth factor secreted by T lymphocytes (1). It stimulates the growth and differentiation of T cells, B cells, NK cells, LAK cells, monocytes, macrophages, and oligodendrocytes (2-4). High-affinity receptors are expressed mainly on activated T cells and macrophages (5), which infiltrate tumors, inflammatory tissues, and autoimmune tissues (6). Peripheral blood cells normally express very low levels of IL-2 receptor (7). ^123^I-IL-2 has been developed as a single photon emission computed tomography (SPECT) tracer for imaging activated immune cells in tumors and pathological tissues (8, 9).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=123I%20and%20Interleukin-2%20and%20synthesis)]

IL-2 was commonly labeled with sodium [^123^I]iodide by electrophilic radioiodination using the chloramine-T method (8). This method gave a radiochemical yield of 16% and a radiochemical purity of >98% in a specific activity of 3.0-4.4 MBq/65 pmol (80-120 μCi/65 pmol). IL-2 was later labeled with lactoperoxidase and glucose oxidase (10) to provide a radiochemical yield of 23.8 ± 9.8% and a radiochemical purity of >98% in a specific activity of 3.7-6.1 MBq/65 pmol (100-165 μCi/65 pmol). [^123^I]IL-2 was purified by column chromatography or high-performance liquid chromatography (HPLC).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=123I%20and%20IL-2%20AND%20in%20vitro)]

^123^I-IL-2 (200 nM) was able to inhibit 90% of the binding of FITC-labeled anti-CD25 (IL-2 receptor) antibody to activated T cells as compared with unlabeled IL-2 (10). The receptor binding capacity of [^123^I]IL-2 was decreased only slightly by the labeling procedure. ^123^I-IL-2 induced proliferation of mitogen-activated human peripheral blood lymphocytes and a murine cytotoxic T lymphocyte cell line, CCTL-2, in a dose-dependent manner (3.7 fM to 1.8 pM). Two classes of ^123^I-IL-2-binding sites (B_max1_ = 2,200 sites/cell, K_d1_ = 500 pM and B_max2_ = 45,000 sites/cell, K_d2_ = 60 nM) were found on the cell surface of activated lymphocytes (11).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=123I%20and%20IL-2%20AND%20rodentia)]

No significant accumulation of ^123^I-IL-2 was observed in major organs except from kidneys and, to a lesser extent, in liver and spleen in normal mice and rats (10). Two animal models to study human autoimmune diabetes were BB/W diabetic rats and Non Obese Diabetic (NOD) mice. In NOD mice receiving injections of labeled IL-2 (65 pmol, 1.2 MBq, 30 μCi per mouse), the pancreatic uptake was 4% injected dose (ID)/g at 2 min after injection and reached a plateau of 8% ID/g at 60 min (12). This trend was not observed in the pancreas of normal mice or in NOD mice receiving injections of labeled α-lactalbumin (65 pmol, 1.2 MBq, 30 μCi per mouse). On the other hand, the uptake in the kidneys and liver decreased with time from the 2-min radioactivity in NOD mice. There was a moderate accumulation of radioactivity in the spleen and thymus with time because of presence of activated lymphocytes in these organs. Planar imaging of NOD and normal mice after ^123^I-IL-2 (130 pmol, 6 MBq, 150 μCi per mouse) injection showed a significant accumulation in the pancreatic region of NOD mice but not in normal mice. Pretreatment of NOD mice with 100 μg of AMT13, an anti-IL-2R antibody, inhibited 30% of pancreatic IL-2 uptake (9). Histological examination of pancreas from NOD and normal mice reveled that there was a significant correlation between the degree of lymphocyte infiltration and radioactivity in the pancreas.

Gamma camera images showed a maximum uptake of ^123^I-IL-2 between 5 and 15 min in pancreas of BB/W rats (10). The other organs with visible uptake were the kidneys and urinary bladder. The retention of radioactivity in the pancreas of BB/W rats was three times higher than the heart at 20 min. In contrast, there was no significant difference between the heart and the pancreas in normal rats. Radioactivity in the spleen was also higher in the BB/W rats than in the normal rats. Histological staining of the pancreas and spleen of BB/W rats confirmed that the degree of infiltration of IL-2R-positive cells was positively correlated with tissue radioactivity.

Infiltrations of activated T cells in rat renal allograft were studied by ^123^I-IL-2 gamma camera imaging (13). The retention of radioactivity at 4 h after injection was 77% of peak activity in rejecting allografts but only 45% in control syngeneic grafts. Retention of radioactivity by rejecting allografts after injection of ^123^I-α-lactalbumin was 36% as nonspecific uptake. Histological and autoradiographic studies showed a positive correlation of the degree of infiltrations of IL-2R-positive cells between allografts and syngeneic controls.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=123I%20and%20IL-2%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=123I%20and%20IL-2%20AND%20%28primate%20NOT%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=123I%20and%20IL-2%20AND%20human)]

Biodistribution of ^123^I-IL-2 was studied in 10 normal volunteers, 10 newly diagnosed, type 1 diabetes patients, 10 coeliac disease patients, and 10 Hashimoto’s thyroiditis patients (11). [^123^I]IL-2 was rapidly cleared from plasma after intravenous injection with t_1/2_ (1) of 1.8 ± 0.7 min and t_1/2_ (2) of 139 ± 26 min. No significant uptake in the thyroid, liver, or gastrointestinal tissues was detectable 1 h after the ^123^I-IL-2 injection in normal subjects. A variable degree of spleen uptake was observed. Significant uptake was detected in the thyroid of all the patients with Hashimoto’s thyroiditis, in the bowel of all the coeliac disease patients, and in the pancreas of all the diabetic patients. ^123^I-IL-2 scintigraphy may be a useful tool for the in vivo assessment of activated mononuclear cell infiltration in various pathological tissues. Internal dosimetry data for ^123^I-IL-2 in humans is not available in the literature.

## Figures, Tables and Boxes Appendix (do not delete)

## References

1 Smith K.A. (1984). Interleukin 2. Annu Rev Immunol.
2 Miyajima A., Miyatake S., Schreurs J., De Vries J., Arai N., Yokota T., Arai K. (1988). Coordinate regulation of immune and inflammatory responses by T cell-derived lymphokines. FASEB J.
3 Muraguchi A., Kehrl J.H., Longo D.L., Volkman D.J., Smith K.A., Fauci A.S. (1985). Interleukin 2 receptors on human B cells. Implications for the role of interleukin 2 in human B cell function. J Exp Med.
4 Smith K.A. (1992). Interleukin-2. Curr Opin Immunol.
5 Smith K.A. (1989). The interleukin 2 receptor. Annu Rev Cell Biol.
6 Signore A., Procaccini E., Annovazzi A., Chianelli M., van der Laken C., Mire-Sluis A. (2000). The developing role of cytokines for imaging inflammation and infection. Cytokine.
7 Robb R.J., Munck A., Smith K.A. (1981). T cell growth factor receptors. Quantitation, specificity, and biological relevance. J Exp Med.
8 Signore A., Beverley P.C., Parman A., Negri M., Pozzilli P. (1987). Labelling of interleukin-2 (IL-2) with 123-iodine with retention of its capacity to bind to activated lymphocytes. Exp Clin Endocrinol.
9 Signore A., Chianelli M., Toscano A., Monetini L., Ronga G., Nimmon C.C., Britton K.E., Pozzilli P., Negri M. (1992). A radiopharmaceutical for imaging areas of lymphocytic infiltration: 123I-interleukin-2. Labelling procedure and animal studies. Nucl Med Commun.
10 Signore A., Chianelli M., Ronga G., Pozzilli P., Beverley P.C. (1990). In vivo labelling of activated T lymphocytes by i.v. injection of 123I-IL2 for detection of insulitis in type 1 diabetes. Prog Clin Biol Res.
11 Signore A., Picarelli A., Annovazzi A., Britton K.E., Grossman A.B., Bonanno E., Maras B., Barra D., Pozzilli P. (2003). 123I-Interleukin-2: biochemical characterization and in vivo use for imaging autoimmune diseases. Nucl Med Commun.
12 Signore A., Chianelli M., Ferretti E., Toscano A., Britton K.E., Andreani D., Gale E.A., Pozzilli P. (1994). New approach for in vivo detection of insulitis in type I diabetes: activated lymphocyte targeting with 123I-labelled interleukin 2. Eur J Endocrinol.
13 Abbs I.C., Pratt J.R., Dallman M.J., Sacks S.H. (1994). Dynamics of the expression of the interleukin-2 (IL-2) receptor in rat renal allografts analyzed by immunohistology, autoradiography, and nuclear imaging using radioiodinated IL-2 probes. Transplantation.